# ^124^I-Labeled anti-CD20 scFv-sc fragment

Chemical name: | ^124^I-Labeled anti-CD20 scFV-sc fragment
Abbreviated name: | [^124^I]Anti-CD20 ScFv-sc DM
Synonym:
Agent Category: | Antibody
Target: | CD-20
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/P11836.1?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_021950.3?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=human+CD20) for information regarding human CD20.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-CD20+minibody)]

The B cell differentiation antigen (CD20) is a transmembrane, non-glycosylated, hydrophobic protein that is characteristically expressed in more than 90% of non-Hodgkin lymphoma (NHL) tumors. Although the exact cellular functions of CD20 are not known, it is believed to play a role in B cell growth, activation, and maintenance of cellular calcium homeostasis (1). Because of its specific presence in the NHL tumor cells, CD20 is targeted with the antibody (Ab) retuximab (http://www.cancer.gov/cancertopics/druginfo/rituximab), which has been approved by the United States Food and Drug Administration (FDA) for use in monotherapy or in combination with a chemotherapeutic agent for the treatment of this disease (2). For enhanced efficacy, radionuclide-coupled anti-CD20 Abs tositumomab (http://us.gsk.com/products/assets/us_bexxar.pdf) (^131^I labeled) or ibritumomab (http://www.cancer.gov/drugdictionary/?CdrID=38483) (^90^Y conjugated) were also respectively approved by the FDA for the treatment of NHL and are commercially available in the United States. In addition, several anti-CD20 Abs, alone or in combination with different chemotherapeutic agents, are under evaluation for the treatment of various cancers in clinical trials (http://clinicaltrials.gov/ct2/results?term=anti+CD-20+antibodies&pg=1) approved by the FDA. In addition, Abs labeled with different nuclides have been used to detect and monitor cancers using imaging techniques such as positron emission tomography (PET) and single-photon emission computed tomography, but, due to long circulation and clearance times of the radiolabeled macromolecules (~150 kDa in size), investigators must wait for awhile before target/background ratios were reduced to suitable levels for imaging purposes (3, 4).

To circumvent the imaging problems encountered with intact radiolabeled Abs, two recombinant retuximab fragments, scFv-C_H_3 (a minibody; ~80 kDa in size) and a double mutant (DM) scFv-Fc fragment (~105 kDa in size, for more information see (4)), were generated, labeled with ^124^I, and evaluated by Olafsen et al. for in vivo imaging of human CD20-expressing lymphomas in mice (3). In this chapter, the biodistribution and imaging characteristics of the ^124^I-labeled scFv-sc fragment ([^124^I]-scFv-sc DM) are described and compared with those of a ^124^I-labeled scFv-C_H_3 minibody ([^124^I]-scFv-C_H_3) used under the same experimental conditions. The biodistribution and imaging characteristics of [^124^I]-scFv-C_H_3 are described and compared with those of ^64^Cu-labeled scFv-C_H_3 in a separate chapter of MICAD (www.micad.nih.gov) (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+CD-20+minibody+production)]

The production, purification, and labeling of scFv-sc DM and scFv-C_H_3 with ^124^I were described by Olafsen et al. (3). The efficiency of radioiodination of scFv-sc DM and scFv-C_H_3 was reported to be 84.9% and 80.9%, respectively, as determined with an instant thin-layer chromatography kit. The specific activities of [^124^I]-scFv-sc DM and [^124^I]-scFv-C_H_3 were reported to be 0.066 MBq/μg (1.78 μCi/μg) and 0.069 MBq/μg (1.86 μCi/μg), respectively. The stability and storage conditions used for [^124^I]-scFv-sc DM and [^124^I]-scFv-C_H_3 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-cd20+minibody+in+vitro+studies)]

The binding of scFv-sc DM to CD20 was confirmed with an indirect immunofluorescence cell-surface staining method using 38C13-huCD20 cells (murine B cell lymphoma 38C13 cells transfected with and expressing the human CD20 gene), as detailed by Olafsen et al. (3) For this study, retuximab was used as a positive control. The binding characteristics of scFv-sc DM were reported to be the same as retuximab.

The immunoreactivity of [^124^I]-scFv-sc DM was determined by exposing an excess number of 38C13-huCD20 cells (the exact number of cells used for the assay was not reported) as described by Olafsen et al. (3). Immunoreactivity of the radiolabeled minibody was reported to be 32.8% compared with 37.7% reported for [^124^I]-scFv-C_H_3. Although immunoreactivity of the radioiodinated Ab fragment was low, the investigators showed that [^124^I]-scFv-sc could easily target CD20-expressing tumors under in vivo conditions (see below).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-cd20+minibody+rodentia)]

The biodistribution and tumor targeting of [^124^I]-scFv-sc DM were investigated in mice bearing either 38C13-huCD20 (expressing CD20) or 38C13 (not expressing CD20) cell tumors (n = 4 animals/cell type) (3). The animals were intravenously injected with the radiolabeled Ab fragment and euthanized 4 h and 21 h later (by 21 h no background was apparent in the tumors and organs and only the CD20 positive tumors showed a strong signal) to study biodistribution of the tracer by retrieving the tumors and other major organs. Accumulated radioactivity in the different tissue types was presented as decay-corrected percent injected dose per gram tissue (% ID/g). The average uptake of radioactivity in the CD20-positive tumors at 21 h after the treatment was reported to be 6.0 ± 2.0% ID/g compared with the significantly lower (P = 0.007) accumulation of label in the CD20-nonexpressing tumors (1.6 ± 0.6% ID/g). With [^124^I]-scFv-C_H_3, the average uptake of label at 21 h after the treatment was reported to be 12.9 ± 3.4% ID/g in the CD20-positive tumors, and a significantly lower (P = 0.003) amount of label accumulated in the CD20-nonexpressing tumors (1.9 ± 0.5% ID/g). Compared with the CD20-positive tumors, a significantly lower (P = 0.05) uptake of radioactivity (<2.0% ID/g) was observed in the liver, spleen, kidneys, and the lungs. A similar observation was made with the radioiodinated minibody. With [^124^I]-scFv-sc DM, the radioactivity uptake ratio of the CD20-positive/CD20-negative tumors was reported to be 3.9 ± 0.7 (this ratio was 7.0 ± 3.1 with the minibody), and the CD20-positive tumor/blood ratio was 3.1 ± 1.2 (this ratio was 4.7 ± 1.4 with [^124^I]-scFv-C_H_3) at 21 h after injection of the label. No blocking studies were reported with either the labeled Ab fragment or the minibody.

Whole-body imaging of the animals was performed at 4 h and 21 h after injection of the radioiodinated scFv-sc DM (3). On the basis of a region of interest (ROI) analysis of the images, only the CD20-positive tumors were reported to have accumulated radioactivity with the labeled Ab fragment at 21 h after treatment. The ROI analysis of the images also revealed that the CD20-positive/CD20-negative tumor ratios with [^124^I]-scFv-sc DM were 1.2 ± 0.2 at 4 h and 2.4 ± 0.8 at 21 h. With [^124^I]-scFv-C_H_3, these ratios were 2.2 ± 0.8 and 4.0 ± 0.7 at the same time points, indicating that the uptake of label by the CD20-positive tumors was higher with the minibody than with the Ab fragments. With [^124^I]-scFv-sc DM, the CD20-positive tumor/soft tissue ratio increased from 4.3 ± 1.4 at 4 h to 9.9 ± 4.6 at 21 h, and these ratios followed a similar but higher pattern with [^124^I]-scFv-C_H_3 (4.6 ± 0.4 and 17.0 ± 6.7 at 4 h and 21 h, respectively). No blocking studies were reported with either the labeled Ab fragment or the minibody.

With results obtained from these studies, the investigators concluded that the labeled anti-CD20 Ab fragments and the labeled minibody could be used for in vivo imaging in rodents, although the labeled minibody yielded images with a better contrast than the Ab fragments (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-cd20+minibody+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

Studies reported in this chapter were supported by National Institutes of Health grants P50 CA107399, P50 CA086306, and CA119367 and a National Cancer Institute grant R24 CA86307.

## References

1 Cragg M.S., Walshe C.A., Ivanov A.O., Glennie M.J. (2005). The biology of CD20 and its potential as a target for mAb therapy. Curr Dir Autoimmun.
2 Bonavida B. (2007). Rituximab-induced inhibition of antiapoptotic cell survival pathways: implications in chemo/immunoresistance, rituximab unresponsiveness, prognostic and novel therapeutic interventions. Oncogene.
3 Olafsen T., Betting D., Kenanova V.E., Salazar F.B., Clarke P., Said J., Raubitschek A.A., Timmerman J.M., Wu A.M. (2009). Recombinant anti-CD20 antibody fragments for small-animal PET imaging of B-cell lymphomas. J Nucl Med.
4 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
5 Chopra, A., [124I/64Cu] Labeled anti-CD20scFv-CH3 minibody [[124I/64Cu]Anti-CD20scFv-CH3]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.